# [^18^F]Fluorobenzaldehyde-leptin

Chemical name: | [^18^F]Fluorobenzaldehyde-leptin
Abbreviated name: | [^18^F]FBA-Leptin
Synonym:
Agent category: | Polypeptide
Target: | Leptin receptor
Target category: | Receptor
Method of detection: | PET
Source of signal\contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3952) for more information about leptin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+Leptin)]

Leptin is secreted by white adipose tissue as a negative feedback response to maintain body weight by regulating appetite and fat metabolism (1). Leptin receptors (ObRs) are present in the brain (the choroid plexus and hypothalamus) and many peripheral tissues, such as the lungs, kidneys, adrenals, and lymph nodes (2, 3). There are at least six types of ObRs (a, b, c, d, e, and f). Administration of leptin is able to correct obesity in humans and in ob/ob obese mice that lack a functional leptin gene (ob) (4). However, a lack of responsiveness to leptin could lead to obesity. An ability to predict altered ObR biodistribution may provide imaging opportunities by the design of specific molecular imaging agents to target ObRs. Flavell et al. (5) introduced an aminooxy group at the C-terminus of leptin using expressed protein ligation technique for labeling with 4-[^18^F]fluorobenzaldehyde ([^18^F]FBA) to synthesize [^18^F]FBA-leptin to image ObRs.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+Leptin+synthesis)]

[^18^F]FBA was added to a solution of 30 nmol aminooxy-leptin in 100 mM anilinium acetate (5). The mixture was incubated for 15 min at 0°C. The resulting product, [^18^F]FBA-leptin, was purified with two spin columns. A decay-corrected yield of 25% based on [^18^F]FBA and a radiochemical purity of >95% were obtained. The specific activity of was 9.25–16.65 MBq/nmol (0.25–0.45 mCi/nmol) with a total synthesis time of 120 min. [^18^F]FBA-Leptin was stable in buffers and mouse serum after 1 h incubation.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+Leptin+in+vitro)]

In vitro binding tests showed that binding of [^18^F]FBA-leptin to cells expressing ObRs was inhibited by 90% with 5 µM leptin (5).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+Leptin+%20rodentia)]

Flavell et al. (5) performed a preliminary study of positron emission tomography analysis in ob/ob mice after intravenous injection of 3.7 MBq (100 μCi) [^18^F]FBA-leptin. [^18^F]FBA-Leptin rapidly accumulated in the cortex of the kidneys. No blocking experiment was performed. The authors noted that further investigation of the biodistribution of [^18^F]FBA-leptin is being performed in various leptin-sensitive and leptin-resistant animal models.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+Leptin+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+Leptin+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+Leptin+human)]

No publication is currently available.

## NIH Support

GM072015, GM55843, GM07739

## References

1 Prieur, X., Y.C. Tung, J.L. Griffin, I.S. Farooqi, S. O'Rahilly, and A.P. Coll, Leptin regulates peripheral lipid metabolism primarily through central effects on food intake. Endocrinology, 2008
2 Bjorbaek C., Kahn B.B. (2004). Leptin signaling in the central nervous system and the periphery. Recent Prog Horm Res.
3 Margetic S., Gazzola C., Pegg G.G., Hill R.A. (2002). Leptin: a review of its peripheral actions and interactions. Int J Obes Relat Metab Disord.
4 Maffei M., Halaas J., Ravussin E., Pratley R.E., Lee G.H., Zhang Y., Fei H., Kim S., Lallone R., Ranganathan S., et al. (1995). Leptin levels in human and rodent: measurement of plasma leptin and ob RNA in obese and weight-reduced subjects. Nat Med.
5 Flavell R.R., Kothari P., Bar-Dagan M., Synan M., Vallabhajosula S., Friedman J.M., Muir T.W., Ceccarini G. (2008). Site-specific (18)F-labeling of the protein hormone leptin using a general two-step ligation procedure. J Am Chem Soc.